# ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-(GSG)-ANTPCGPYTHDCPVKR

Chemical name: | ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-(GSG)-ANTPCGPYTHDCPVKR
Abbreviated name: | ^111^In-DOTA(GSG)-G3-C12
Synonym:
Agent category: | Peptide
Target: | Galectin-3
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=2385452), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=2385451) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3958) for more information about galectin-3.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20galectin-3)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Galectin-3 (Gal-3) is a carbohydrate-binding protein (30 kDa) with a highly conserved carbohydrate recognition domain (CRD) at the C-terminus (4). Gal-3 is found not only on the cell surface but also in the cytoplasm and nucleus. It is also secreted into the extracellular space. Gal-3 is involved in multiple biological conditions such as cellular adhesion, apoptosis, differentiation, metastasis, and inflammation. Gal-3 is found to be overexpressed in various human cancer cells with even higher expression in metastatic cancer cells (5, 6). Interactions of Gal-3 with certain carbohydrates and ECM proteins promote tumor cell adhesion and metastasis through inhibition of tumor cell apoptosis and induction of endothelial cell proliferation and angiogenesis (7-11). The peptide ANTPCGPYTHDCPVKR (G3-C12) was identified to be a selective binder to Gal-3 with phage display screening, and G3-C12 inhibits adhesion of tumor cells to endothelial cells (12). Kumar et al. (13) introduced the linker GSG to the N-terminus alanine (A) of the G3-C12 peptide for conjugation with tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (DOTA) for labeling with ^111^In. ^111^In-DOTA(GSG)-G3-C12 has been evaluated as a single-photon emission computed tomography (SPECT) agent for Gal-3 expression in tumors in vivo (13, 14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20galectin-3%20and%20synthesis)]

DOTA-(GSG)-G3-C12 was prepared with solid-phase peptide synthesis (13). DOTA-(GSG)-G3-C12 was purified with reverse-phase high-performance liquid chromatography. Radiolabeling was performed by mixing ^111^InCl_3_ in ammonium acetate with DOTA-(GSG)-G3-C12. The mixture was heated at 85°C for 30 min. The radiochemical purity and specific activity of ^111^In-DOTA-(GSG)-G3-C12 were >98% and 68.5 GBq/µmol (1.9 Ci/µmol), respectively. The labeling yield was 30%. ^111^In-DOTA-(GSG)-G3-C12 was stable in saline for 12 h and mouse serum for 30 min with some degradation at the later time points.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20galectin-3+and+in+vitro)]

An in vitro receptor-binding assay of ^111^In-DOTA-(GSG)-G3-C12 was performed on Gal-3–expressing human MDA-MB-435 breast cancer cell line (13). Binding of ^111^In-DOTA-(GSG)-G3-C12 to Gal-3 was ~5% of the incubation dose after 60 min of incubation at 37°C, whereas the control ^111^In-DOTA-(GSG)-G3-C12 scrambled peptide showed no appreciable binding. ^111^In-DOTA-(GSG)-G3-C12 was not internalized into the cells. In-DOTA-(GSG)-G3-C12 exhibited a 50% inhibition concentration (IC_50_) of 200.0 ± 6.7 nM. Deutscher et al. (14) reported that In-DOTA-(GSG)-G3-C12 inhibited ^111^In-DOTA-(GSG)-G3-C12 binding to human PC3-M prostate carcinoma cells with an IC_50_ value of 191 ± 10.2 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20galectin-3%20and%20rodentia)]

Kumar et al. (13) performed ex vivo biodistribution studies of ^111^In-DOTA-(GSG)-G3-C12 in nude mice (n = 3/group) bearing a human MDA-MB-435 breast tumor. Each mouse received 0.11 MBq (3 nCi) ^111^In-DOTA-(GSG)-G3-C12 by intravenous injection. The tumor radioactivity levels were 1.02 ± 0.75% injected dose per gram (ID/g) at 30 min, 0.75 ± 0.05% ID/g at 1 h, 0.60 ± 0.04% ID/g at 2 h, and 0.16 ± 0.04% ID/g at 4 h. The accumulation in the tumor was inhibited by 48% with pretreatment of excess non-labeled In-DOTA-(GSG)-G3-C12 (P < 0.01) at 2 h after tracer injection. The accumulation of the tracer was the highest in the kidney (25.9% ID/g), followed by the intestine (0.52% ID/g), lung (0.49% ID/g), blood (0.31% ID/g), and liver (0.25% ID/g) at 1 h after injection. The urine contained 88.6% ID at 1 h after injection. The peak tumor/blood and tumor/muscle ratios were 8.6 and 30.0 at 2 h, respectively. Whole-body SPECT imaging was performed at 2 h after ^111^In-DOTA-(GSG)-G3-C12 injection. The tumor and kidneys were the only tissue/organ clearly visualized. On the other hand, only the kidneys were visualized with the injection of ^111^In-DOTA-(GSG)-G3-C12 scrambled peptide. Deutscher et al. (14) showed similar ex vivo biodistribution and SPECT imaging results with human PC3-M prostate tumor-bearing SCID mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20galectin-3+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20galectin-3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20galectin-3+and+human)]

No publication is currently available.

## NIH Support

P50 CA103130-01

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Barondes S.H., Cooper D.N., Gitt M.A., Leffler H. (1994). Galectins. Structure and function of a large family of animal lectins. J Biol Chem.
5 Takenaka Y., Fukumori T., Raz A. (2004). Galectin-3 and metastasis. Glycoconj J.
6 Raz A., Zhu D.G., Hogan V., Shah N., Raz T., Karkash R., Pazerini G., Carmi P. (1990). Evidence for the role of 34-kDa galactoside-binding lectin in transformation and metastasis. Int J Cancer.
7 Wang, Y., P. Nangia-Makker, L. Tait, V. Balan, V. Hogan, K.J. Pienta, and A. Raz, Regulation of Prostate Cancer Progression by Galectin-3. Am J Pathol, 2009
8 Nakahara S., Raz A. (2008). Biological modulation by lectins and their ligands in tumor progression and metastasis. Anticancer Agents Med Chem.
9 Nakahara S., Raz A. (2007). Regulation of cancer-related gene expression by galectin-3 and the molecular mechanism of its nuclear import pathway. Cancer Metastasis Rev.
10 Fukumori T., Takenaka Y., Oka N., Yoshii T., Hogan V., Inohara H., Kanayama H.O., Kim H.R., Raz A. (2004). Endogenous galectin-3 determines the routing of CD95 apoptotic signaling pathways. Cancer Res.
11 Nangia-Makker P., Honjo Y., Sarvis R., Akahani S., Hogan V., Pienta K.J., Raz A. (2000). Galectin-3 induces endothelial cell morphogenesis and angiogenesis. Am J Pathol.
12 Zou J., Glinsky V.V., Landon L.A., Matthews L., Deutscher S.L. (2005). Peptides specific to the galectin-3 carbohydrate recognition domain inhibit metastasis-associated cancer cell adhesion. Carcinogenesis.
13 Kumar S.R., Deutscher S.L. (2008). 111In-labeled galectin-3-targeting peptide as a SPECT agent for imaging breast tumors. J Nucl Med.
14 Deutscher S.L., Figueroa S.D., Kumar S.R. (2009). Tumor targeting and SPECT imaging properties of an (111)In-labeled galectin-3 binding peptide in prostate carcinoma. Nucl Med Biol.